# ^68^Ga-Labeled (4-{[(bis(phosphonomethyl))carbamoyl]methyl}-7,10-bis(carboxymethyl)-1,4,7,10-tetraazacyclododec-1-yl)acetic acid (BPAMD)

Chemical name: | ^68^Ga-Labeled (4-{[(bis(phosphonomethyl))carbamoyl]methyl}-7,10-bis(carboxymethyl)-1,4,7,10-tetraazacyclododec-1-yl)acetic acid (BPAMD)
Abbreviated name: | [^68^Ga]BPAMD
Synonym:
Agent Category: | Compound
Target: | Hydroxyapatite; farnesyl diphosphate synthase
Target Category: | Others (bone); enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on structure of [^68^Ga]BPAMD for more information in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Bisphosphonates&cmd=DetailsSearch)]

Bisphosphonates (BPs; also known as diphosphonates), such as methylene diphosphonate (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=38ac7426-d447-4327-b8c7-9e438d562865) (MDP) and zoledronic acid (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=3c79ff9c-a6f4-405d-b19c-7e473a61dedc), can be labeled with technetium-99m ([^99m^Tc]-BPs) for bone scintigraphy (gamma planar imaging or single-photon emission computed tomography (SPECT)) to detect osteoporosis and other skeletal-related events (SREs), including bone metastases (1). These chemicals are known to promote osteoclast apoptosis and have a strong affinity for hydroxyapatite, a component of the bone matrix. The exact mechanism of action of these bone-seeking compounds is described in detail elsewhere (2-4). Although the ^99m^Tc-labeled compounds have high sensitivity, selectivity, and accuracy for the detection of SREs, they are known to generate some false positive and false negative results in the clinic (5). [^18^F]-Fluoride is another nuclide that is commonly used for bone imaging with positron emission tomography (PET) and is believed to be superior to [^99m^Tc]-BPs for the diagnosis of SREs (6). However, the main limitations of using ^18^F are the requirement of a cyclotron to produce it and the high costs that are associated with the production of this radionuclide (5). In an effort to develop an imaging compound that does not have the limitations of tracers that are currently used to detect SREs with scintigraphy or PET, a bisphosphonate labeled with ^68^Ga was developed and shown to be potentially useful for imaging the mouse skeletal system with PET (5).

The main advantage of using ^68^Ga (half-life = 68 min; β^+^ = 89%; E+_βmax_ = 1.9 MeV) for bone imaging over either ^99m^Tc (half-life = 6 h; γ^+^ = 100%; E+_γmax_ = 140 keV) or ^18^F (half-life = ~110 min; β^+^ = 97%; E+_βmax_ = 0.635 MeV) as a radiolabel is that ^68^Ga can be produced economically on-site with a ^68^Ge/^68^Ga generator (5, 7). In addition, images obtained with PET have a higher spatial resolution compared with those obtained with SPECT (7). In an ongoing effort to develop a compound that could be used for the targeted imaging of bone metastases, a novel 1,4,7,10-tetraazacyclododecane-N,N',N,N'-tetraacetic acid (DOTA) derivative that contained a bisphosphonate within its structure ((4-{[(bis(phosphonomethyl))carbamoyl]methyl}-7,10-bis(carboxymethyl)-1,4,7,10-tetraazacyclododec-1-yl)acetic acid (BPAMD)) was developed (8, 9), labeled with ^68^Ga ([^68^Ga]BPAMD), and shown to be suitable for the imaging of bone metastases in mice (7) and humans (10).

### Related Resource Links

Related chapters (http://www.ncbi.nlm.nih.gov/books/?term=MDP+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) in MICAD

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_001037277.1) of human farnesyl diphosphate synthase

Gene information (http://www.ncbi.nlm.nih.gov/gene/2224) regarding human farnesyl diphosphate synthase (GeneID: 2224)

Farnesyl diphosphate synthase in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim/134629) database

Structure of farnesyl diphosphate synthase (http://www.ncbi.nlm.nih.gov/Structure/mmdb/mmdbsrv.cgi?uid=59201) complexed with a bisphosphonate

Farnesyl diphosphate synthase in Kyoto Encyclopedia of Genes and Genomes (KEGG) Pathways (http://www.genome.jp/dbget-bin/www_bget?pathway+hsa00900)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=bisphosphonates) with bisphosphonates (or diphosphonates)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=BPAMD%20synthesis&cmd=DetailsSearch)]

The synthesis of BPAMD is described elsewhere (8, 9). The labeling of BPAMD with ^68^Ga was initially optimized for the concentration of the ligand (BPAMD), pH, time, and temperature as detailed by Fellner et al. (7). The radiochemical yield of the labeling reaction was reported to be 90%, and the radiochemical purity of the final product after purification was >98% as determined with high-performance liquid chromatography. The specific activity of [^68^Ga]BPAMD was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=68Ga%20BPAMD%20in%20vitro%20studies&cmd=DetailsSearch)]

The in vitro binding characteristics of [^68^Ga]BPAMD were studied by exposing the radiochemical to commercially available synthetic hydroxyapatite (Hap) (7). The binding of [^68^Ga]BPAMD to the matrix was reported as the percent of ^68^Ga absorbed to Hap and determined to be 81.5 ± 0.5% within 10 min at ambient temperature.

The stability of [^68^Ga]BPAMD was investigated (n = 5 studies) by incubating the probe in the presence or absence of apo-transferrin (39.2 nmol/mL) in phosphate-buffered saline (PBS; pH 7.4) for 3 h at 37°C (7). Thin-layer chromatographic analysis showed that 4.2 ± 0.8% of ^68^Ga had transchelated by the end of the incubation when it was incubated with PBS alone, whereas 9.1 ± 0.6% of 68Ga had transchelated in the presence of apo-transferrin during the same time period.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=68Ga%20BPAMD%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^68^Ga]BPAMD was studied in a healthy rat by administering 15 MBq (555 μCi) of the radiochemical through the tail vein of the animals (7). Dynamic PET scans of the rodent were acquired for 60 min postinjection (p.i.) From the images it was apparent that maximum radioactivity was present in the shoulder joints and certain areas of the vertebral column of the animal that show a relatively high remodeling activity. In the backbone, the accumulation of label in the humerus, sternum, and scapula was 2.49-fold, 2.88-fold, and 2.08-fold higher, respectively, compared with the solid bone. This indicated that the tracer accumulated preferentially in those areas of the skeleton that exhibited a high metabolic activity in the animals. No blocking studies were reported.

In another study, rats were injected with Walker 256 cells (http://www.cell-lines-service.de/content/e174/e158/e2031/e1724/index_eng.html) to induce bone metastases in the rodents (7). Two weeks later, the animals (n = 7 rats) were injected with 20.5 ± 0.5 MBq (758.5 ± 18.5 μCi) [^68^Ga]BPAMD to evaluate the use of this tracer for the visualization of metastatic lesions in the skeletal system of the rats. Whole-body PET scans acquired from the animals at 60–70 min p.i. showed that only five animals had developed metastasis in the tibia. The lesions were reported to accumulate 3.97 ± 1.82-fold higher radioactivity (n = 4 rats) compared with a healthy area of the bone that served as an intraindividual control. Presence of osteolytic metastasis in the tibia of the animals was confirmed with histological examination of the tissue.

From these studies, the investigators concluded that [^68^Ga]BPAMD can be used for the detection of bone metastases in rodents (7).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=68Ga%20BPAMD%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=68Ga%20BPAMD%20Non-Human%20Primates&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=68Ga%20BPAMD%20Human%20Studies&cmd=DetailsSearch)]

A patient known to have extensive bone metastasis of prostate cancer was intravenously injected with 462 MBq (~17 mCi) [^68^Ga]BPAMD (10). Whole-body PET images of the individual revealed that the radioactivity had accumulated in multiple lesions of the vertebrae, ribs, and the proximal extremities of the patient. For comparison, PET images were also acquired from the patient after injection of 270 MBq (~10 mCi) [^18^F]-fluoride, and the images showed that the metastatic lesions were present in the entire skeletal system of the patient as observed with [^68^Ga]BPAMD. With [^68^Ga]BPAMD, the maximal standardized uptake values (SUV_max_) of the tenth and twelfth vertebrae were 77.1 and 62.1, respectively, compared with the SUV_max_ values of 39.1 and 39.2, respectively, obtained with ^18^F. This indicated that [^68^Ga]BPAMD was probably superior to ^18^F for the visualization of bone metastasis in humans (10).

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Lin J., Luo S., Chen C., Qiu L., Wang Y., Cheng W., Ye W., Xia Y. (2010). Preparation and preclinical pharmacological study on a novel bone imaging agent (99m)Tc-EMIDP. Appl Radiat Isot.
2 Kimmel D.B. (2007). Mechanism of action, pharmacokinetic and pharmacodynamic profile, and clinical applications of nitrogen-containing bisphosphonates. J Dent Res.
3 Zhang Y., Cao R., Yin F., Hudock M.P., Guo R.T., Krysiak K., Mukherjee S., Gao Y.G., Robinson H., Song Y., No J.H., Bergan K., Leon A., Cass L., Goddard A., Chang T.K., Lin F.Y., Van Beek E., Papapoulos S., Wang A.H., Kubo T., Ochi M., Mukkamala D., Oldfield E. (2009). Lipophilic bisphosphonates as dual farnesyl/geranylgeranyl diphosphate synthase inhibitors: an X-ray and NMR investigation. J Am Chem Soc.
4 Mitterhauser M., Toegel S. (2011). Radiopharmaceutical considerations on bone seeker uptake: should we learn from therapeutical targets of bisphosphonates?. Nucl Med Biol.
5 Suzuki K., Satake M., Suwada J., Oshikiri S., Ashino H., Dozono H., Hino A., Kasahara H., Minamizawa T. (2011). Synthesis and evaluation of a novel 68Ga-chelate-conjugated bisphosphonate as a bone-seeking agent for PET imaging. Nucl Med Biol.
6 Kruger S., Buck A.K., Mottaghy F.M., Hasenkamp E., Pauls S., Schumann C., Wibmer T., Merk T., Hombach V., Reske S.N. (2009). Detection of bone metastases in patients with lung cancer: 99mTc-MDP planar bone scintigraphy, 18F-fluoride PET or 18F-FDG PET/CT. Eur J Nucl Med Mol Imaging.
7 Fellner M., Biesalski B., Bausbacher N., Kubicek V., Hermann P., Rosch F., Thews O. (2012). (68)Ga-BPAMD: PET-imaging of bone metastases with a generator based positron emitter. Nucl Med Biol.
8 Kubicek V., Rudovsky J., Kotek J., Hermann P., Vander Elst L., Muller R.N., Kolar Z.I., Wolterbeek H.T., Peters J.A., Lukes I. (2005). A bisphosphonate monoamide analogue of DOTA: a potential agent for bone targeting. J Am Chem Soc.
9 Vitha T., Kubicek V., Hermann P., Elst L.V., Muller R.N., Kolar Z.I., Wolterbeek H.T., Breeman W.A., Lukes I., Peters J.A. (2008). Lanthanide(III) complexes of bis(phosphonate) monoamide analogues of DOTA: bone-seeking agents for imaging and therapy. J Med Chem.
10 Fellner M., Baum R.P., Kubicek V., Hermann P., Lukes I., Prasad V., Rosch F. (2010). PET/CT imaging of osteoblastic bone metastases with (68)Ga-bisphosphonates: first human study. Eur J Nucl Med Mol Imaging.